# (3-Ethyl-2-[^11^C]methyl-6-quinolinyl)(cis-4-methoxycyclohexyl)methanone

Chemical name: | (3-Ethyl-2-[^11^C]methyl-6-quinolinyl)(cis-4-methoxycyclohexyl)methanone
Abbreviated name: | [^11^C]JNJ-16567083
Synonym: | [^11^C]2
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C%20JNJ-16567083)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, with low density in the cerebellum. mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) radioligands targeting mGluR5 can visualize and analyze mGluR5 expression in normal physiological and pathological conditions. However, only a few mGluR1 ligands have been studied. (3-Ethyl-2-methyl-6-quinolinyl)(cis-4-methoxycyclohexyl)methanone (JNJ-16567083) was shown to be a selective mGluR1 antagonist with nanomolar affinity (K_i_ = 0.87 nM) with little inhibition of mGluR5 (5). Huang et al. (5) prepared and evaluated (3-Ethyl-2-[^11^C]methyl-6-quinolinyl)(cis-4-methoxycyclohexyl)methanone ([^11^C]JNJ-16567083) for use with in vivo PET imaging of mGluR1 distribution in rat brain.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JNJ-16567083%20and%20synthesis)]

Huang et al. (5) synthesized [^11^C]JNJ-16567083 by methylation of the trimethyltin precursor with [^11^C]methyl iodide ([^11^C]MeI) at 120°C for 5 min. Subsequent separation with high-performance liquid chromatography produced a radiochemical purity >99%. An average radiochemical yield was 47 ± 17% (n = 10) based on [^11^C]MeI. The specific activity of [^11^C]JNJ-16567083 was 22.5 ± 8.4 GBq/μmol (607 ± 228 mCi/µmol) at the end of synthesis. The total synthesis time was 40 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JNJ-16567083%20and%20in%20vitro)]

JNJ-16567083 exhibited K_i_ values of 0.87 ± 0.43 nM and 2.4 ± 0.6 µM for rat mGluR1 and mGluR5 (5), respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JNJ-16567083%20and%20rodentia)]

Huang et al. (5) performed ex vivo biodistribution studies in the brain of rats (n = 3/group) at 10, 30, and 60 min after intravenous injections of [^11^C]JNJ-16567083. The initial accumulation of radioactivity was high in the brain and thereafter decreased. The cerebellum exhibited the highest accumulation of radioactivity at 10 min with 1.24 ± 0.06% injected dose/gram (ID/g), followed by the striatum (0.73 ± 0.04% ID/g), hippocampus (0.58 ± 0.05% ID/g), frontal cortex (0.52 ± 0.06% ID/g), medulla (0.47 ± 0.01% ID/g), and blood (0.42 ± 0.02% ID/g). The cerebellum/medulla ratios were 2.63, 4.72, and 4.06 at 10, 30, and 60 min, respectively. Pretreatment with JNJ-16567083 (2 mg/kg, 10 min) reduced the radioactivity in the cerebellum by 81% and in the striatum, hippocampus and frontal cortex by 50% at 30 min after injection.

Huang et al. (5) performed dynamic PET imaging studies in one rat after intravenous injection of 4.4 MBq (0.12 mCi) [^11^C]JNJ-16567083 for 90 min. Blocking studies were performed by co-injection of excess JNJ-16567083. Baseline tissue time-activity curves revealed a high accumulation of radioactivity peaked at 10 min in the cerebellum, with a moderate radioactivity levels in the striatum, hippocampus and cerebral cortex. Co-injection of JNJ-16567083 reduced the radioactivity in the all brain regions to homogeneous level.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JNJ-16567083%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JNJ-16567083%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20JNJ-16567083%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Huang Y., Narendran R., Bischoff F., Guo N., Zhu Z., Bae S.A., Lesage A.S., Laruelle M. (2005). A positron emission tomography radioligand for the in vivo labeling of metabotropic glutamate 1 receptor: (3-ethyl-2-[11C]methyl-6-quinolinyl)(cis- 4-methoxycyclohexyl)methanone. J Med Chem.